# Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-gold nanoparticles

Chemical name: | Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-gold nanoparticles
Abbreviated name: | Cy5.5-MMP-AuNPs
Synonym:
Agent category: | Peptide
Target: | Matrix metalloproteinases (MMPs)
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/contrast: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20AuNPs)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Gold has not been used as an X-ray contrast agent in vivo. Gold has a higher atomic number and a higher absorption coefficient than iodine, providing 2.7-fold greater contrast/weight than iodine (4). Furthermore, imaging gold at 80–100 keV reduces interference from bone absorption and provides lower soft tissue absorption, which would reduce radiation to patients. Hainfeld et al. (4) used gold nanoparticles (AuNPs; 1.9 nm in diameter, ~50 kDa) as a computed tomography (CT) contrast agent in mice; these experiments showed enhanced CT contrast of the vasculature, kidneys, and tumor in mice. However, plasma proteins in blood adsorb onto the surface of bare AuNPs, which produces large aggregates (5) that may result in altered pharmacokinetics and biodistribution of AuNPs (6). Polyethylene glycol (PEG) has been found to minimize nonspecific adsorption of proteins onto NPs and to reduce their uptake by the liver (6). PEG-AuNPs have been being studied as cancer CT imaging and photothermal agents (7).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis and tumor invasion and metastases (8-11). MMP expression in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages, is highly regulated. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (12). The peptide Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-NH_2_ was found to be a MMP substrate and is cleaved between Leu and Gly residues. Lee et al. (13) used this sequence with a Cy5.5 NIR dye molecule to attach to AuNPs to form fluorescence-quenched nanoparticles (Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-AuNPs (Cy5.5-MMP-AuNPs)). The Cy5.5 molecules are in close proximity, which results in fluorescence quenching because of efficient fluorescence resonance energy transfer to Au. The NIR fluorescence signal increases when the Leu-Gly bond is cleaved by MMPs, releasing Cy5.5-containing fragments. Cy5.5 is a NIR fluorescent dye with absorbance maximum at 675 nm and emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. Cy5.5-MMP-AuNPs are being developed for NIR fluorescence imaging of MMPs expressed in tumors, atherosclerosis, myocardial infarction, and other diseases.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20AuNPs)]

Lee et al. (13) prepared Cy5.5-MMP-AuNPs by coating of Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys to AuNPs. Cy5.5 mono OSu ester (4.8 µmol) was conjugated to the N-termimus of Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys at room temperature for 2 h. Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys(amide) was purified with HPLC. Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys(amide) was incubated with AuNPs in 0.01 M phosphate buffer containing 0.1% SDS and 0.3 M NaCl for 24 h. The Cy5.5-MMP-AuNPs were purified with repeated washing and centrifugation. The purified nanoparticles were ~20 nm in diameter as measured with transmission electron microscopy. There were ~114 molecules of Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys per AuNP. The quenching efficiency of a single AuNP was calculated to be >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20AuNPs%20and%20in%20vitro)]

Lee et al. (13) showed that Cy5.5-MMP-AuNPs (14 nM) were activated by MMP-2, MMP-3, MMP-7, and MMP-13 in a time-dependent manner with NIR fluorescence signal increases of 13.9-, 12.2-, 16.5-, and 24.4-fold, respectively, after 120 min of incubation. Co-incubation of MMP-2 with a MMP-2–selective inhibitor (1 mM, 1,10-phenanthrolone) markedly reduced NIR fluorescence signal from a 13.9-fold enhancement to a 3.3-fold enhancement.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20AuNPs%20and%20rodentia)]

Lee et al. (13) performed biodistribution studies of Cy5.5-MMP-AuNPs administered to mice bearing human SCC7 squamous cell carcinoma (MMP-2–positive) cell line via intratumoral injection (the injected dose was not reported). Optical imaging was performed for 4 h after injection. A good NIR fluorescence signal was visualized at 0.5 h and increased ~two-fold at 4 h as compared with the signal at 0.5 h. The tumor signal was reduced ~80% with pretreatment with the MMP-2 inhibitor (30 min before injection with Cy5.5-MMP-AuNPs). The tumor/tissue ratio was 7.0 for the probe and 2.5 for the probe pretreated with the MMP-2 inhibitor. Intramuscular injection of the probe in normal mice did not provide a stronger signal than the surrounding background tissue. Histoimmunological staining of tumor and tissue sections revealed strong expression of MMP-2 in the tumor cells with colocalization of NIR fluorescence signal.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20AuNPs%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20AuNPs%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20AuNPs%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Hainfeld J.F., Slatkin D.N., Focella T.M., Smilowitz H.M. (2006). Gold nanoparticles: a new X-ray contrast agent. Br J Radiol.
5 Zhang F., Skoda M.W., Jacobs R.M., Zorn S., Martin R.A., Martin C.M., Clark G.F., Goerigk G., Schreiber F. (2007). Gold nanoparticles decorated with oligo(ethylene glycol) thiols: protein resistance and colloidal stability. J Phys Chem A.
6 Otsuka H., Nagasaki Y., Kataoka K. (2003). PEGylated nanoparticles for biological and pharmaceutical applications. Adv Drug Deliv Rev.
7 Cai Q.Y., Kim S.H., Choi K.S., Kim S.Y., Byun S.J., Kim K.W., Park S.H., Juhng S.K., Yoon K.H. (2007). Colloidal gold nanoparticles as a blood-pool contrast agent for X-ray computed tomography in mice. Invest Radiol.
8 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
9 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
10 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
11 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
12 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
13 Lee S., Cha E.J., Park K., Lee S.Y., Hong J.K., Sun I.C., Kim S.Y., Choi K., Kwon I.C., Kim K., Ahn C.H. (2008). A near-infrared-fluorescence-quenched gold-nanoparticle imaging probe for in vivo drug screening and protease activity determination. Angew Chem Int Ed Engl.